# ^68^Ga-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC

Chemical name: | ^68^Ga-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC
Abbreviated name: | ^68^Ga-DOTA-MUT-DS
Synonym:
Agent Category: | Affibody, antibody
Target: | HER2
Target Category: | Receptor
Method of detection: | PET
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=affibody%20and%20HER2%20and%20molecular%20imaging)]

The ^68^Ga-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ (MUT-DS) conjugate with a disulfide bridge between the two homocysteines, abbreviated as ^68^Ga-DOTA-MUT-DS, is a 2-helix affibody derivative that was synthesized by Ren et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that are derived from the B-domain of staphylococcal surface protein A (2, 3). These molecules have only 58 amino acid residues (~7 kDa), which form a 3-α-helical bundle structure (3, 4). Helices 1 and 2 bundles are responsible for the high binding affinity and specificity of affibodies to their targets, while helix 3 contributes to the affibody stabilization and is not involved in receptor recognition (4). Studies have further confirmed that the binding domain in the helices 1 and 2 bundles includes 13 amino acid residues that are surface-exposed (2). Therefore, large affibody libraries have been constructed by randomization of the 13 amino acid residues, and a large set of affibody molecules against a wide variety of targets have been selected from those libraries. Of them, the affibodies specific to HER2, including Z_HER2:342_ and Z_HER2:477_, have been intensively investigated in recent years (3, 5). These molecules have been radiolabeled and tested for molecular imaging of HER2-expressing tumors.

The investigators at Stanford University first tested the feasibility of the monomeric (~7 kDa) and dimeric (~14 kDa) forms of affibody Z_HER2:477_ for molecular imaging (6, 7). Both forms have been labeled with various radionuclides through chelating agents. Studies have shown that smaller affibody constructs perform better in vivo in terms of tumor uptake and clearance, which prompts them to generate smaller proteins with only α-helices 1 and 2 bundles (~4 kDa) (4, 6, 7). However, simple deletion of the helix 3 leads to significantly decreased binding affinity of the proteins because of decreased helix conformation (4). The investigators then applied various strategies to improve the helix conformation of the affibody molecules, including sequence mutation, placement of disulfide bridges, and inclusion of helix-promoting amino acids (4). Although the helix conformation (~15%, the amount of α-helix represented in the secondary structure of the affibodies) of the 2-helix molecules is still much lower than that of the parent 3-helix affibodies, the investigators successfully obtained a class of 2-helix small proteins with HER2-binding affinity up to 5 nM with these strategies (1, 8, 9). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles with a disulfide bridge being formed between the two inserted homocysteines (4). The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for imaging HER2-expressing tumors. ^68^Ga-DOTA-MUT-DS, ^64^Cu-DOTA-MUT-DS, ^111^In-DOTA-MUT-DS, and ^18^F-FBO-MUT-DS are examples of the MUT-DS derivatives (1, 8, 9).

This chapter summarizes the data obtained with ^68^Ga-DOTA-MUT-DS (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/).

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19690041)]

Ren et al. generated the cyclic 2-helix small protein MUT-DS with standard solid-phase peptide synthesis and I_2_ oxidation of the two inserted homocysteines (1). DOTA was conjugated to the C-terminus cysteine residule. The DOTA-MUT-DS conjugate was purified with high-performance liquid chromatography (HPLC). The chemical yield was 10%, with >95% purity. The retention time was 19.1 min. The measured molecular weight was 5,136.77 (calculated 5,136.53).

DOTA-MUT-DS was then radiolabeled with ^68^Ga through the reaction with ^68^GaCI_3_ in 0.1-N NH_4_OAc for 20 min at 75°C (1). After purification, the labeled ^68^Ga-DOTA-MUT-DS had a >95% radiochemical purity and a 35%−56% radiochemical yield. The retention time was 19.1 min on HPLC. Because the unlabeled DOTA-MUT-DS could not be separated from ^68^Ga-DOTA-MUT-DS, Ren et al. obtained a modest specific activity of 2.65–3.69 MBq/nmol (71.62–99.73 μCi/nmol) at the end of synthesis. The intact radiolabeled complex maintained >90% after incubation for 40 min with mouse serum at 37°C, indicating good in vitro stability.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19690041)]

The binding affinity of DOTA-MUT-DS with the extracellular domain of HER2 antigen was measured in vitro with surface plasmon resonance detection and was determined to be 4.76 nM, which is the same as unmodified MUT-DS (5 nM) (1, 4). This result suggests that DOTA conjugation did not alter the binding affinity of the 2-helix protein. DOTA-MUT-DS displayed a fast on-rate (association constant, 1.62 × 10^5^ s^-1^) and a slow off-rate (dissociation constant, 7.7 × 10^-4^ s^-1^).

The HER2-targeting ability for cultured cells was evaluated with SKOV3 human ovarian cancer cells after incubation for 0.5–2 h with 6.29 kBq (0.17 μCi) ^68^Ga-DOTA-MUT-DS (1). The probe quickly accumulated in the SKOV3 cells and reached 1.76 ± 0.22% of applied activity at 0.5 h, which increased to 3.19 ± 0.31% at 1 h and then slightly dropped to 2.57 ± 0.48% at 2 h. In the presence of a large excess of nonradioactive Z_HER2:477_ (1 µg), the cell uptake of the probe was significantly inhibited at all incubation time points (P < 0.05), being only 0.17 ± 0.07% at 1 h and <0.1% at 2 h. These results suggest that ^68^Ga-DOTA-MUT-DS is specific to HER2.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19690041)]

The biodistribution of ^68^Ga-DOTA-MUT-DS was examined in mice bearing SKOV3 human ovarian tumors after tail vein injection of 0.296 MBq (8 μCi) probe (1). Mice were euthanized at 0.5, 1, and 2 h after injection (n = 3 mice/time point). Rapid accumulation of the probe in tumors was observed at early time points (2.55 ± 0.72% injected dose per gram tissue (ID/g) at 0.5 h after injection), which continually increased to 4.04 ± 0.24% ID/g at 2 h after injection. ^68^Ga-DOTA-MUT-DS also displayed rapid blood clearance of 1.78 ± 0.68% at 0.5 h to 0.77 ± 0.2% and 0.60 ± 0.11% ID/g at 1 h and 2 h, respectively. The tumor/blood ratio was 1.59 ± 0.7 at 0.5 h, increased to 5.32 ± 0.18 at 1 h, and maximized at 7.72 ± 2.1 at 2 h. The tumor/muscle ratio maximized at 1 h (9.94 ± 1.29). Of the major organs, the liver uptake was 1.14 ± 0.19% ID/g at 0.5 h and decreased to 0.85 ± 0.09% ID/g at 2 h. The lung uptake was 1.76 ± 0.61% ID/g at 0.5 h and 0.67 ± 0.14% ID/g at 2 h. Kidney uptake was >200% ID/g at all time points. All other major organs showed low uptake (<1.10% ID/g at 1 h) and fast clearance.

The in vivo tumor-targeting specificity was evaluated with pretreatment of tumor-bearing mice with 17-N,N-dimethyl ethylene diamine-geldanamycin (17-DMAG; 50 mg/kg every 8 h before imaging, three times) (1). The compound 17-DMAG is known for its inhibition of HER2 signaling by binding to an Hsp90 chaperone protein. Inhibition of HER2 expression by 17-DMAG was confirmed by Ren et al. with Western blot studies. Pretreatment significantly reduced the tumor uptake of ^68^Ga-DOTA-MUT-DS at 2 h after injection to ~32% of the corresponding uptake in untreated tumors (4.12 ± 0.83 versus 0.74 ± 0.23% ID/g; P < 0.01). Consequently, the tumor/blood ratio was significantly decreased with 17-DMAG pretreatment (7.72 ± 2.1 versus 1.69 ± 0.16; P < 0.01). The liver and kidney uptake also decreased with 17-DMAG pretreatment (P < 0.05).

PET images were obtained from a mouse bearing a SKOV3 tumor at 0.5, 1, and 2 h after tail vein injection of ^68^Ga-DOTA-MUT-DS (1). The SKOV3 tumor was clearly visible with good tumor/background contrast. High accumulation of radioactivity was also seen in the kidneys. Pretreatment with 17-DMAG at 24 h before imaging made tumors hardly visible at any time points. The tumor uptake of ^68^Ga-DOTA-MUT-DS was significantly lower in the treated mice than in the untreated mice (n = 3 mice/group per time point; P < 0.01).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
5 Gao J., Chen K., Miao Z., Ren G., Chen X., Gambhir S.S., Cheng Z. (2011). Affibody-based nanoprobes for HER2-expressing cell and tumor imaging. Biomaterials.
6 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
7 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
8 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.
9 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011